# 1R-[^11^C]Phenylephrine

Chemical name: | 1R-[^11^C]Phenylephrine
Abbreviated name: | [^11^C]PHEN
Synonym: | (−)-[^11^C]Phenylephrine
Agent Category: | Compound
Target: | Norepinephrine transporter (NET), vesicular monoamine transporter (VMAT2), neuronal storage vesicle, monoamine oxidase (MAO)
Target Category: | Transporter binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C-11-PHEN%20OR%20%5B11C%5DPhenylephrine%20OR%20%5B11C%5D-%28-%29-Phenylephrine)]

1R-[^11^C]Phenylephrine ([^11^C]PHEN) is a radioligand developed for positron emission tomography (PET) imaging of the sympathetic nervous system (SNS). It is a catecholamine analog labeled with ^11^C, a positron emitter with a physical t_½_ of 20.4 min (1, 2).

Many diseases affect the SNS, and imaging of the pathologic changes of adrenergic transmission has been an important area of PET research (3, 4). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter, norepinephrine (NE), which stimulates adrenergic receptors in various effector organs (5). There are different types of adrenergic receptors, and NE stimulates α_1_, β_1_ and certain β_2_ receptors. The NE transporter (NET) is a transmembrane protein located in the adrenergic nerve terminals that is responsible for active reuptake (uptake-1) of NE released by neurons (6). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS such as the heart and brain. There is substantial evidence that aberrations in cardiac SNS function contribute to the morbidity and mortality associated with cardiac diseases (7).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. meta-Iodobenzylguanidine ([^123^]MIBG), a single-photon emission tomography (SPECT) agent, has been developed and used for neuronal imaging (2). Efforts have been made to develop a positron-emitting tracer because of the inadequate quantitative information and lower spatial resolution obtained by SPECT imaging with MIBG. [^11^C]meta-Hydroxyephedrine ([^11^C]mHED) was first developed based on metaraminol, a synthetic false transmitter analog of NE, that accumulates in nerve terminals in the same way as NE (8). [^11^C]PHEN is structurally similar to [^11^C]mHED and lacks only the α-methyl group. This difference appears to render [^11^C]PHEN susceptible to oxidative deamination by axoplasmic monoamine oxidase (MAO). Thus, [^11^C]PHEN is transported into sympathetic nerve varicosities by NET and taken up into storage vesicles (9, 10). It is most likely cleaved by MAO at the α-carbon into two by-products: an unlabeled aldehyde and [^11^C]methylamine. [^11^C]Methylamine is a freely diffusible molecule that rapidly leaves the neuron and enters the systemic circulation. In principle, heart PET imaging with [^11^C]PHEN may allow the assessment of heart MAO activity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DPhenylephrine%20AND%20synthesis)]

Del Rosario et al. (1) synthesized [^11^C]PHEN from the precursor of (−)-m-octopamine. (±)-m-Octopamine was obtained commercially and converted to the anhydrous free-base form with use of O,O-dibenzoyl (+)-tartartic acid for separation. Repeated recrystallization produced (−)-m-octopamine as the dibenzoyl (+)-tartrate salt with >94-96% enantiomeric purity. (−)-m-Octopamine was methylated with either CH_3_I or CF_3_SO_3_^11^CH_3_. For best yield, Del Rosario et al. (1) trapped gaseous CF_3_SO_3_^11^CH_3_ at −40 °C in a solution of (−)-m-octopamine (~1 mg/300 µl in anhydrous dimethylformamide). The mixture was warmed to room temperature in 2 min and then purified by strong cation-exchange high-performance liquid chromatography (HPLC). The specific activity was >18,500 GBq (500 Ci)/mmol at the end of synthesis (EOS). Radiochemical yield was >50% at EOS, and radiochemical purity was >97%. Chiral purity was >94-96%, as determined by copper Schiff-base chiral HPLC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DPhenylephrine%20AND%20in%20vitro)]

Raffel et al. (11) studied the metabolism and kinetics of [^11^C]PHEN in in vitro-isolated working rat hearts. [^11^C]PHEN with a specific activity >18,500 GBq (500 Ci)/mmol at EOS was used. [^11^C]D2-PHEN, a [^11^C]PHEN analog with deuterium replacement of the two hydrogen atoms on the α-carbon of the PHEN side chain to slow MAO activity at the tracer level, was used in the experiment. The initial uptake rates (K_up_, ml/min/g wet weight) for [^11^C]PHEN (n = 11) and [^11^C]D2-PHEN (n = 6), were not significantly different: 0.72 ± 0.15 and 0.82 ± 0.10, respectively. Treatment with pargyline (100 µM; MAO inhibitor) did not change the uptake rate of [^11^C]PHEN, but treatment with reserpine (vesicular uptake inhibitor) decreased the uptake rates of both [^11^C]PHEN and [^11^C]D2-PHEN. The washout half-times (sum of three exponential terms) for [^11^C]PHEN and [^11^C]D2-PHEN were significantly different: 98.2 ± 13.7 and 163.2 ± 39.0 min, respectively. In the presence of pargyline, reserpine, and pargyline+reserpine, the t_½_ of [^11^C]PHEN decreased to 140.4 ± 27.8, 31.2 ± 6.0, and 14.9 ± 1.3 min, respectively. In the presence of reserpine, the t_½_ of [^11^C]D2-PHEN decreased to 14.6 ± 3.4 min. The study concluded that [^11^C]PHEN kinetics were sensitive not only to neuronal MAO activity but also to changes in neuronal vesicular storage function.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DPhenylephrine%20AND%20rodentia)]

A tissue distribution study of [^11^C]PHEN in rats was conducted by Del Rosario et al. (1) with a dose of 2.7-5.4 kBq (100-200 µCi). At 30 min, major organs with high radioactivity were the heart, liver, and spleen. The percent of injected dose per g (% ID/g) values for the ventricles, liver, lung, spleen, kidney, and blood at 30 min were 1.45 ± 0.25, 1.51 ± 0.15, 0.62 ± 0.09, 1.30 ± 0.20, 1.01 ± 0.31, and 0.23 ± 0.02, respectively. Approximately 2.44% ID accumulated in the submaxillary gland at 30 min. More than 50% of the radioactivity present in the heart at 5 min was cleared from the heart by 60 min. In comparison, [^11^C]PHEN showed lower initial heart uptake and faster heart clearance than [^11^C]mHED. The study also showed that [^3^H]phenylephrine (^3^H on position 4 of the phenyl ring) and [^11^C]PHEN had similar heart efflux rates. Very low brain extraction (0.06% ID) at 30 min was observed. Pretreatment with desipramine (DMI), a specific blocker, showed blockade for the ventricles and atria ranging from 72 to 77%. After treatment with clorgyline, a selective MAO (isoform A) inhibitor, the heart radioactivity levels were higher at 15 and 60 min than those in untreated rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DPhenylephrine%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Del Rosario et al. (1) reported the heart time-activity curves and PET images of [^11^C]PHEN in dogs. PET heart images at 30-60 min indicated relatively fast clearance of radioactivity from the heart. The time−activity profile in dogs appeared to be similar to that in rats. Raffel et al. (10) reported no significant differences between the kinetics of [^11^C]PHEN and [^11^C]D2-PHEN in dogs. The authors suggested that there was considerable species variability in cardiac MAO and that MAO levels in the canine heart were very low. Thus, dogs could be a problematic animal model for studying MAO sensitivity.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DPhenylephrine%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DPhenylephrine%29%20AND%20human)]

Raffel et al. (9) performed cardiac PET studies with [^11^C]PHEN in 14 healthy volunteers. The specific activity of [^11^C]PHEN was >18.5 TBq (500 Ci)/mmol at EOS, and the dose was 740 MBq (20 mCi). Tandem studies with [^11^C]mHED were performed in 10 patients. The relative myocardial distributions of [^11^C]PHEN and [^11^C]mHED were similar, but [^11^C]PHEN cleared from the myocardium with an average t_½_ of 58 ± 5.2 min, whereas [^11^C]mHED activity remained constant for the 40-60 min of imaging time. The retention index (tissue activity/arterial blood activity ratio, as ml blood/min/ml tissue, based on PET images) values of [^11^C]PHEN were approximately half those of [^11^C]mHED. These values were significantly correlated when corrections for blood [^11^C]PHEN metabolites (appeared at approximately 3 times the rate of [^11^C]mHED) were made. After oral DMI oral administration (two 50-mg doses), there were marked decreases in myocardial activity of both radioligands. Mean reductions of both radioligands were not significantly different.

In another study, Raffel and Wieland (10) conducted paired PET experiments with [^11^C]PHEN and [^11^C]D2-PHEN in 6 normal volunteers. The retention indexes at 40-60 min for [^11^C]PHEN and [^11^C]D2-PHEN were 0.066 ± 0.011 and 0.086 ± 0.018, respectively. The washout half-times for [^11^C]PHEN and [^11^C]D2-PHEN were 59 ± 10 and 155 ± 52 min, respectively. The authors concluded that the in vivo kinetics of [^11^C]PHEN were sensitive to neuronal MAO activity in the human heart. Because vesicular storage of [^11^C]PHEN protected it from MAO metabolism, [^11^C]PHEN kinetics were also dependent on vesicular storage function.

## NIH Support

NIH HL 27555, NIH R01-HL47543, R01-27555.

## References

1 Del Rosario R.B., Jung Y.W., Caraher J., Chakraborty P.K., Wieland D.M. (1996). Synthesis and preliminary evaluation of [11C]-(-)-phenylephrine as a functional heart neuronal PET agent. Nucl Med Biol.
2 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
3. Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
4. Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
5. Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
6 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
7 Caldwell J.H., Kroll K., Li Z., Seymour K., Link J.M., Krohn K.A. (1998). Quantitation of presynaptic cardiac sympathetic function with carbon-11-meta-hydroxyephedrine. J Nucl Med.
8 Rosenspire K.C., Haka M.S., Van Dort M.E., Jewett D.M., Gildersleeve D.L., Schwaiger M., Wieland D.M. (1990). Synthesis and preliminary evaluation of carbon-11-meta-hydroxyephedrine: a false transmitter agent for heart neuronal imaging. J Nucl Med.
9 Raffel D.M., Corbett J.R., del Rosario R.B., Gildersleeve D.L., Chiao P.C., Schwaiger M., Wieland D.M. (1996). Clinical evaluation of carbon-11-phenylephrine: MAO-sensitive marker of cardiac sympathetic neurons. J Nucl Med.
10 Raffel D.M., Corbett J.R., del Rosario R.B., Mukhopadhyay S.K., Gildersleeve D.L., Rose P., Wieland D.M. (1999). Sensitivity of [11C]phenylephrine kinetics to monoamine oxidase activity in normal human heart. J Nucl Med.
11 Raffel D.M., Wieland D.M. (1999). Influence of vesicular storage and monoamine oxidase activity on [11C]phenylephrine kinetics: studies in isolated rat heart. J Nucl Med.